# Anti-vascular cell adhesion molecule antibody M/K-2.7–conjugated microparticles of iron oxide

Chemical name: | Anti-vascular cell adhesion molecule antibody M/K-2.7–conjugated microparticles of iron oxide
Abbreviated name: | VCAM-MPIO
Synonym: | M/K-2.7-MPIO
Agent category: | Antibody
Target: | Vascular cell adhesion molecule-1 (VCAM-1)
Target category: | Antigen
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=54648638), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=46249772) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=7412) for more information about VCAM-1.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+MPIO+Selectin)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules, which comprise >80% of most soft tissues. The contrast of proton MRI images depends mainly on the nuclear density (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the use of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide nanoparticles and other iron oxide formulations affect T2 primarily and lead to a decreased signal. On the other hand, paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

Endothelial cells have important roles in inflammatory responses (2, 3). Bacterial lipopolysaccharide (LPS), virus, inflammation, and tissue injury increase tumor necrosis factor α (TNFα), interleukin-1 (IL-1), and other cytokine and chemokine secretion. Emigration of leukocytes from blood is dependent on their ability to roll along endothelial cell surfaces and subsequently adhere to endothelial cell surfaces. Inflammatory mediators and cytokines induce chemokine secretion from endothelial cells and other vascular cells and increase their expression of cell-surface adhesion molecules, such as intracellular adhesion molecule-1 (ICAM-1), vascular cell adhesion molecule-1 (VCAM-1), integrins, and selectins. Chemokines are chemotactic toward leukocytes and toward sites of inflammation and tissue injury. The movement of leukocytes through endothelial junctions into the extravascular space are highly orchestrated through various interactions with different adhesion molecules on endothelial cells (4).

VCAM-1 is found in very low levels on the cell surface of resting endothelial cells and other vascular cells, such as smooth muscle cells and fibroblasts (5-9). VCAM-1 binds to very late antigen-4 (VLA-4) integrin on the cell surface of leukocytes. IL-1 and TNFα increase expression of VCAM-1, P-selectin, and other cell adhesion molecules on the vascular endothelial cells, which leads to leukocyte adhesion to the activated endothelium. Furthermore, VCAM-1 expression is induced by oxidized low-density lipoproteins under atherogenic conditions (10). Overexpression of VCAM-1 by atherosclerotic lesions plays an important role in their progression toward vulnerable plaques, which may erode and rupture. Microparticles of iron oxide (MPIO) are composed of iron particles with a diameter of ~4.5 µm. MPIO targeted with anti-VCAM-1 monoclonal antibody (mAb) M/K-2.7 (VCAM-MPIO) is being developed as a non-invasive agent for VCAM-1 expression in vascular endothelial cells during different stages of inflammation in atherosclerosis and renal ischemia (11).

### Related Resource Links:

- Chapters in MICAD (VCAM-1 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=VCAM-1+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (VCAM-1 (http://www.ncbi.nlm.nih.gov/gene/7412))
- Articles in Online Mendelian Inheritance in Man (OMIM) (VCAM-1 (http://www.ncbi.nlm.nih.gov/omim/192225))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+MPIO+Selectin+synthesis)]

The synthesis of VCAM-MPIO was described by McAteer et al. (12). The p-toluenesulphonyl-MPIO (diameter, 1 µm) was purchased commercially (Invitrogen). The M/K-2.7 mAb (33 pmol/10^7^ MPIO) was incubated with activated MPIO for 20 h at 37°C. IgG control MPIO (IgG-MPIO) was prepared in the same way with 33 pmol M/K-2.7 mAb. MPIO was washed and incubated with 0.1% bovine serum albumin for 4 h at 37°C to block the remaining activated sites. The number of antibodies per MPIO was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+MPIO+Selectin+in+vitro)]

McAteer et al. (12) performed in vitro cell-binding assays with VCAM-MPIO using mouse sEND-1 endothelial cells. As determined with light microscopy, VCAM-MPIO bound to only TNF-activated sEND-1 cells (R^2^ = 0.94; P = 0.03) in a dose-dependent manner, whereas IgG-MPIO did not. A corresponding decrease in MRI signal intensity of the MPIO was observed on 11.7-T MRI images (R^2^ = 0.98, P = 0.01), indicating the presence of VCAM-MPIO on the cell surface. VCAM-MPIO binding was blocked by preincubation with soluble VCAM-1 and not by ICAM-1. Unconjugated MPIO was phagocytosed by mouse peritoneal macrophages and not by sEND-1 cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+MPIO+Selectin+rodentia)]

Akhtar et al. (11) performed MRI (9.4 T) with VCAM-MPIO in a renal ischemia reperfusion injury (IRI) mouse model. The left renal pedicle was ligated for 30 min with subsequent perfusion for 16–18 h and injection of 4.5 mg iron/kg VCAM-MPIO (n = 5 mice) or IgG-MPIO (n = 3 mice). MRI was performed at 0, 30, 60, and 90 min after MPIO injection with automated segmentation and quantification of contrast volume. There was a rapid increase in contrast volume at 30 min and maximal contrast by 60 min in the IRI kidneys, with sequestration in the spleen and liver. IRI kidneys (5,991 ± 354 × 10^6^ µm^3^) showed a 69-fold increase, but a decrease in signal in VCAM-MPIO contrast compared to the control kidneys (87 ± 7 × 10^6^ µm^3^; P < 0.001). IgG-MPIO showed minimal accumulation (~100 × 10^6^ µm^3^) in the IRI and control kidneys. Pretreatment with anti-VCAM-1 antibody (1.32 nmol/kg, 15 min) blocked VCAM-MPIO accumulation by ~90% to 625 ± 80 × 10^6^ µm^3^. VCAM-1 expression in the IRI kidneys was 65-fold higher than in the control kidneys and in significant (P < 0.01) correlation with VCAM-MPIO contrast volume (R^2^ = 0.90). Histological examination of the IRI kidney sections showed that VCAM-MPIO adhered to the vessel walls of the peritubular capillaries and was not associated with local infarction and renal tubules.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+MPIO+Selectin+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+MPIO+Selectin+(primate%20not%20human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+MPIO+Selectin+human)]

No publication is currently available.

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Cybulsky M.I., Gimbrone M.A. (1991). Endothelial expression of a mononuclear leukocyte adhesion molecule during atherogenesis. Science.
3 Lowe J.B. (2002). Glycosylation in the control of selectin counter-receptor structure and function. Immunol Rev.
4 Vanderslice P., Woodside D.G. (2006). Integrin antagonists as therapeutics for inflammatory diseases. Expert Opin Investig Drugs.
5 Bochner B.S., Luscinskas F.W., Gimbrone M.A., Newman W., Sterbinsky S.A., Derse-Anthony C.P., Klunk D., Schleimer R.P. (1991). Adhesion of human basophils, eosinophils, and neutrophils to interleukin 1-activated human vascular endothelial cells: contributions of endothelial cell adhesion molecules. J Exp Med.
6 Kume N., Cybulsky M.I., Gimbrone M.A. (1992). Lysophosphatidylcholine, a component of atherogenic lipoproteins, induces mononuclear leukocyte adhesion molecules in cultured human and rabbit arterial endothelial cells. J Clin Invest.
7 Leung K.H. (1999). Release of soluble ICAM-1 from human lung fibroblasts, aortic smooth muscle cells, dermal microvascular endothelial cells, bronchial epithelial cells, and keratinocytes. Biochem Biophys Res Commun.
8 Luscinskas F.W., Cybulsky M.I., Kiely J.M., Peckins C.S., Davis V.M., Gimbrone M.A. (1991). Cytokine-activated human endothelial monolayers support enhanced neutrophil transmigration via a mechanism involving both endothelial-leukocyte adhesion molecule-1 and intercellular adhesion molecule-1. J Immunol.
9 Nagel T., Resnick N., Atkinson W.J., Dewey C.F., Gimbrone M.A. (1994). Shear stress selectively upregulates intercellular adhesion molecule-1 expression in cultured human vascular endothelial cells. J Clin Invest.
10 Aikawa M., Libby P. (2004). The vulnerable atherosclerotic plaque: pathogenesis and therapeutic approach. Cardiovasc Pathol.
11 Akhtar, A.M., J.E. Schneider, S.J. Chapman, A. Jefferson, J.E. Digby, K. Mankia, Y. Chen, M.A. McAteer, K.J. Wood, and R.P. Choudhury, In vivo quantification of VCAM-1 expression in renal ischemia reperfusion injury using non-invasive magnetic resonance molecular imaging. PLoS One, 20105(9): p. e12800 (1-10).
12 McAteer M.A., Schneider J.E., Ali Z.A., Warrick N., Bursill C.A., von zur Muhlen C., Greaves D.R., Neubauer S., Channon K.M., Choudhury R.P. (2008). Magnetic resonance imaging of endothelial adhesion molecules in mouse atherosclerosis using dual-targeted microparticles of iron oxide. Arterioscler Thromb Vasc Biol.